# 4-[^18^F]Fluoro-N-[4-[6-(isopropylamino)pyrimidin-4-yl]-1,3-thiazol-2-yl]-N-methylbenzamide

Chemical name: | 4-[^18^F]Fluoro-N-[4-[6-(isopropylamino)pyrimidin-4-yl]-1,3-thiazol-2-yl]-N-methylbenzamide
Abbreviated name: | [^18^F]FITM, [^18^F]4
Synonym:
Agent category: | Compound
Target: | Metabotropic glutamate receptor subtype 1 (mGluR1)
Target category: | Receptor
Method of detection: | Positron emission tomography (PET)
Source of signal: | ^18^F
Activation: | No
Studies: | - In vitro; - Rodents; - Non-human primates | Click on the above structure for additional information in PubChem (http://pubchem.ncbi.nlm.nih.gov/).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=FITM)]

Glutamate is a major excitatory neurotransmitter at neuronal synapses in the central nervous system (CNS) (1, 2). Glutamate produces its excitatory effects by acting on cell-surface ionotropic glutamate or metabotropic glutamate receptors (mGluRs). The mGluRs are GTP-binding protein (G-protein)–coupled receptors that play important roles in regulating the activity of many synapses in the CNS, and many neuronal projection pathways contain mGluRs. There are eight mGluR subtypes, which are further subdivided into groups I, II, and III. The group I receptors include mGluR1 and mGluR5, and they are found predominantly in postsynaptic locations. The mGluR1 is found in moderate to high density in the cerebellum, caudate, putamen, thalamus, cingulate cortex, and hippocampus, with low density in the pons. The mGluR5 is usually found in moderate to high density in the frontal cortex, caudate, putamen, nucleus accumbens, olfactory tubercle, and hippocampus, whereas the density in the cerebellum is low. The mGluR1 and mGluR5 are positively coupled to phospholipase C in the regulation of neuronal excitability (3). Dysfunction of mGluR1 and mGluR5 is implicated in a variety of diseases in the CNS, including anxiety, depression, schizophrenia, Parkinson’s disease, and drug addiction or withdrawal (2, 4).

Positron emission tomography (PET) radioligands targeting mGluR1 can visualize and analyze mGluR1 expression in normal physiological and pathological conditions (5-8). Several radioligands have been studied for in vivo imaging of mGluR1 in the brain. 4-Fluoro-N-[4-[6-(isopropylamino)pyrimidin-4-yl]-1,3-thiazol-2-yl]-N-methylbenzamide (FITM) was shown to be a selective mGluR1 antagonist with nanomolar affinity (K_i_ = 5.4 nM), with little inhibition to mGluR2, mGluR5, and mGluR8 (9). Yamasaki and colleagues (10-12) prepared and evaluated 4-[^18^F]Fluoro-N-[4-[6-(isopropylamino)pyrimidin-4-yl]-1,3-thiazol-2-yl]-N-methylbenzamide ([^18^F]FITM) for use with in vivo PET imaging of mGluR1 distribution in the brains of small animals and monkeys.

### Related Resource Links:

- Chapters in MICAD (mGluR1 (http://www.ncbi.nlm.nih.gov/books?Db=books&Cmd=DetailsSearch&Term=mGluR1+AND+micad%5Bbook%5D), mGluR5 (http://www.ncbi.nlm.nih.gov/books?term=mGluR5%20AND%20micad%5Bbook%5D))
- Gene information in NCBI (mGluR1 (http://www.ncbi.nlm.nih.gov/gene/2911), mGluR5 (http://www.ncbi.nlm.nih.gov/gene/2915))
- Articles in Online Mendelian Inheritance in Man (OMIM) (mGluR1 (http://omim.org/entry/604473), mGluR5 (http://www.ncbi.nlm.nih.gov/omim/604102))
- Clinical trials (mGluR1 (http://www.clinicaltrials.gov/ct2/results?term=mGluR1), mGluR5 (http://www.clinicaltrials.gov/ct2/results?term=mglur5))

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=FITM%20and%20synthesis)]

Yamasaki et al. (12) reported a one-step automated synthesis of [^18^F]FITM. The nitro-precursor was subjected to nucleophilic fluorination with K[^18^F]F/Kryptofix2.2.2 for 10 min at 180°C, with a radiochemical yield of 14 ± 3% (n = 8) and a specific activity of 204–559 GBq/μmol (5.5–15.1 Ci/μmol) after purification with high-performance liquid chromatography. The radiochemical purity of [^18^F]FITM was >99%. The total synthesis time was not reported. [^18^F]FITM exhibited a log D_7.4_ value of 1.46 ± 0.01.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=FITM%20and%20in%20vitro)]

In vitro [^18^F]FITM autoradiographic imaging studies were performed on rat brain sections (n = 3/group) (12). [^18^F]FITM bound heterogeneously to the brain sections, with the highest accumulation of radioactivity in the mGluR1-rich thalamus (739 ± 67 PSL/mm^2^) and cerebellum (719 ± 209 PSL/mm^2^), followed by the hippocampus (681 ± 16 PSL/mm^2^), striatum (568 ± 15 PSL/mm^2^), cerebral cortex (375 ± 50 PSL/mm^2^), and pons (222 ± 77 PSL/mm^2^). FITM and JNJ-16259685 (1,000 nM, mGluR1 antagonists) completely blocked radioactive signals to background levels in these brain regions. On the other hand, the mGluR5 antagonist MPEP (1,000 nM) demonstrated only marginal inhibition (5%–18%) of the signals. In vitro autoradiographic studies were also performed on monkey brain sections (n = 6) with results similar to those found with the rat brain sections.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=FITM%20and%20rodentia)]

Yamasaki et al. (12) performed ex vivo autoradiographic studies in rat brain sections (n = 10) that received intravenous injection of [^18^F]FITM with or without co-administration of JNJ-16259685 (1 mg/kg). [^18^F]FITM bound heterogeneously to the brain sections, with the highest accumulation of radioactivity in the mGluR1-rich thalamus (673 ± 38 PSL/mm^2^) and cerebellum (636 ± 26 PSL/mm^2^), followed by the striatum (479 ± 33 PSL/mm^2^), hippocampus (428 ± 17 PSL/mm^2^), cerebral cortex (342 ± 24 PSL/mm^2^), and pons (69 ± 5 PSL/mm^2^). JNJ-16259685 (mGluR1 antagonist) blocked radioactive signals by 86%–91% in the thalamus, cerebellum, striatum, hippocampus, and cerebral cortex, whereas the signal was reduced only 15% in the pons.

Yamasaki et al. (10) performed dynamic PET imaging studies for 90 min in rats (n = 4/group) after intravenous injection of 17.5 MBq (0.5 mCi) [^18^F]FITM. Blocking studies were performed by pretreatment (0.5 min) with 1 mg/kg FITM. Baseline tissue time-activity curves revealed a high accumulation of radioactivity in the cerebellum, followed by the thalamus, striatum, hippocampus, and cingulate cortex, whereas little radioactivity was detected in the pons. Pretreatment with FITM reduced the radioactivity signals to background level with no effect on the blood level of radioactivity. Logan graphic analysis showed baseline volume of distribution (V_T_) values of 114, 59, 48, 50, 42, and 6 ml/mm^3^ for the cerebellum, thalamus, striatum, hippocampus, cingulate cortex, and pons, respectively. Blocking with FITM reduced these V_T_ values to 2.4–2.7 ml/mm^3^. Non-displaceable binding potential (BP_ND_) values were estimated to be 43.9, 22.3, 17.9, 18.6, 15.5, and 1.5, respectively. Pretreatment with various doses of FITM estimated the K_d_ values to be 1.5–2.1 nM for the thalamus, hippocampus, striatum, and cingulate cortex, with B_max_ values of 36.3, 27.5, 22.2, and 20.5 pM, respectively. [^18^F]FITM remained ~25% intact in the plasma at 120 min with two polar metabolites, 1 (69%) and 2 (5%). On the other hand, [^18^F]FITM remained ~96% intact in the brain at 120 min with only metabolite 2 (4%).

Ex vivo biodistribution studies were performed in mice (n = 3/group) at 1–180 min after intravenous injection of [^18^F]FITM (11). The liver and kidney (>7.5% injected dose/gram (ID/g)) exhibited high initial accumulation of radioactivity at 1 min. Radioactivity increased with time in the brain (7.7% ID/g at 15 min) and small intestine (10% ID/g at 60 min), whereas radioactivity decreased with time in the other tissues, such as the lung, spleen, heart, bone, and blood (<2% ID/g at 60 min).

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=FITM%20and%20%28dog%20or%20pig%20or%20sheep%20or%20rabbit%29)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=FITM%20and%20%28primate%20not%20human%29)]

Yamasaki et al. (11) performed dynamic PET imaging studies for 90 min in one male rhesus monkey after intravenous injection of 175 MBq (5 mCi, 0.8 nmol) [^18^F]FITM. Blocking studies were performed by pretreatment (0.5 min) with 3 mg/kg JNJ-16259685. Baseline tissue time-activity curves revealed a high accumulation of radioactivity in the cerebellum, followed by the thalamus, striatum, hippocampus, and cingulate cortex, whereas little radioactivity was detected in the pons. The maximum standard uptake values (SUVs) were 3.3, 2.3, 2.0, 1.9, 1.5, and 1.7 for the cerebellum, cingulate cortex, thalamus, hippocampus, striatum, and putamen, respectively. Pretreatment with JNJ-16259685 reduced the radioactivity signals of all regions to 0.1–0.2 at 90 min after injection. Logan graphic analyses showed baseline V_T_ values of 10.2, 5.9, 5.0, 4.4, 3.4, 3.3, and 2.4 ml/mm^3^ for the cerebellum, cingulate cortex, thalamus, hippocampus, putamen, caudate, and pons, respectively. Similar V_T_ values for these brain regions were obtained with two-tissue compartment model analyses.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=FITM%20and%20human)]

No publication is currently available.

## References

1 Pin J.P., Duvoisin R. (1995). The metabotropic glutamate receptors: structure and functions. Neuropharmacology.
2 Ferraguti F., Crepaldi L., Nicoletti F. (2008). Metabotropic glutamate 1 receptor: current concepts and perspectives. Pharmacol Rev.
3 Abe T., Sugihara H., Nawa H., Shigemoto R., Mizuno N., Nakanishi S. (1992). Molecular characterization of a novel metabotropic glutamate receptor mGluR5 coupled to inositol phosphate/Ca2+ signal transduction. J Biol Chem.
4 Gasparini F., Lingenhohl K., Stoehr N., Flor P.J., Heinrich M., Vranesic I., Biollaz M., Allgeier H., Heckendorn R., Urwyler S., Varney M.A., Johnson E.C., Hess S.D., Rao S.P., Sacaan A.I., Santori E.M., Velicelebi G., Kuhn R. (1999). 2-Methyl-6-(phenylethynyl)-pyridine (MPEP), a potent, selective and systemically active mGlu5 receptor antagonist. Neuropharmacology.
5 Ametamey S.M., Kessler L.J., Honer M., Wyss M.T., Buck A., Hintermann S., Auberson Y.P., Gasparini F., Schubiger P.A. (2006). Radiosynthesis and preclinical evaluation of 11C-ABP688 as a probe for imaging the metabotropic glutamate receptor subtype 5. J Nucl Med.
6 Ametamey S.M., Treyer V., Streffer J., Wyss M.T., Schmidt M., Blagoev M., Hintermann S., Auberson Y., Gasparini F., Fischer U.C., Buck A. (2007). Human PET studies of metabotropic glutamate receptor subtype 5 with 11C-ABP688. J Nucl Med.
7 Baumann C.A., Mu L., Johannsen S., Honer M., Schubiger P.A., Ametamey S.M. (2010). Structure-activity relationships of fluorinated (E)-3-((6-methylpyridin-2-yl)ethynyl)cyclohex-2-enone-O-methyloxime (ABP688) derivatives and the discovery of a high affinity analogue as a potential candidate for imaging metabotropic glutamate recepors subtype 5 (mGluR5) with positron emission tomography (PET). J Med Chem.
8 Honer M., Stoffel A., Kessler L.J., Schubiger P.A., Ametamey S.M. (2007). Radiolabeling and in vitro and in vivo evaluation of [(18)F]-FE-DABP688 as a PET radioligand for the metabotropic glutamate receptor subtype 5. Nucl Med Biol.
9 Satoh A., Nagatomi Y., Hirata Y., Ito S., Suzuki G., Kimura T., Maehara S., Hikichi H., Satow A., Hata M., Ohta H., Kawamoto H. (2009). Discovery and in vitro and in vivo profiles of 4-fluoro-N-[4-[6-(isopropylamino)pyrimidin-4-yl]-1,3-thiazol-2-yl]-N-methylbenzam ide as novel class of an orally active metabotropic glutamate receptor 1 (mGluR1) antagonist. Bioorg Med Chem Lett.
10 Yamasaki T., Fujinaga M., Kawamura K., Yui J., Hatori A., Ohya T., Xie L., Wakizaka H., Yoshida Y., Fukumura T., Zhang M.R. (2012). In Vivo Measurement of the Affinity and Density of Metabotropic Glutamate Receptor Subtype 1 in Rat Brain Using 18F-FITM in Small-Animal PET. J Nucl Med.
11 Yamasaki T., Fujinaga M., Maeda J., Kawamura K., Yui J., Hatori A., Yoshida Y., Nagai Y., Tokunaga M., Higuchi M., Suhara T., Fukumura T., Zhang M.R. (2012). Imaging for metabotropic glutamate receptor subtype 1 in rat and monkey brains using PET with [18F]FITM. Eur J Nucl Med Mol Imaging.
12 Yamasaki T., Fujinaga M., Yoshida Y., Kumata K., Yui J., Kawamura K., Hatori A., Fukumura T., Zhang M.R. (2011). Radiosynthesis and preliminary evaluation of 4-[18F]fluoro-N-[4-[6-(isopropylamino)pyrimidin-4-yl]-1,3-thiazol-2-yl]-N-methylb enzamide as a new positron emission tomography ligand for metabotropic glutamate receptor subtype 1. Bioorg Med Chem Lett.